# Trans-1,2,3,5,6,10b-hexahydro-6-[4-([^18^F]fluoroethylthio)-phenyl]pyrrolo-[2,1-a]-isoquinoline

Chemical name: | Trans-1,2,3,5,6,10b-hexahydro-6-[4-([^18^F]fluoroethylthio)-phenyl]pyrrolo-[2,1-a]-isoquinoline
Abbreviated name: | [^18^F]FEMcN
Synonym:
Agent Category: | Trans-1,2,3,5,6,10b-hexahydro-6-[4-(methylthio)-phenyl]pyrrolo-[2,1-a]-isoquinoline
Target: | Serotonin transporter
Target Category: | Binding
Method of detection: | PET
Source of signal: | ^18^F
Activation: | Not required
Studies: | - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=%5B18F%5DFEMcN&WebEnv=0hK0YmMjA9v3GIwZtSQuh4QaBpDOuHA8U9PiSfQJopb3oTrSNvnFwdsB8bnaZwrOAqlXsOZxZoVlwu%40D475071265C2C690_0024SID&WebEnvRq=1)]

The serotonin (5-HT) system is known to serves as the gastrointestinal signaling molecule (1) and plays an important role in the development of alcohol dependence (2). It is also involved in a variety of physiological functions and has a function in the development of post-meal satiety, and the pathogenesis of epilepsies, Alzheimer’s and Parkinson’s diseases (3-5). It is also known to be involved in the development of anxiety and depression disorders (6). Thus imaging of the 5-HT system is considered important to understand a variety of neurological and psychiatric functions and disorders.

A variety of drugs have been labeled with radioactive iodine (^123^I), carbon (^11^C) or fluorine (^18^F) for imaging of the 5-HT receptor or transporter using the positron emission tomography (PET) technique. Among these, trans-1,2,3,5,6,10b-hexahydro-6-[4-(methylthio)-phenyl]pyrrolo-[2,1-a]-isoquinoline ([^11^C]McN5652-Z), a highly potent serotonin transport (SERT) blocker was developed for imaging and is still used for the evaluation of this system (7, 8). However, during the initial development of [^11^C]McN5652-Z, because ^11^C compounds have a very short half-life (20 min), Suehiro et al. (5) decided to synthesize and evaluate the use of an ^18^F labeled analog of McN5652-Z, that would have a longer half-life, to investigate the SERT system. For this an S-[^18^F]fluoroethyl analog of McN5652-Z, trans-1,2,3,5,6,10b-hexahydro-6-[4-([^18^F]fluoroethylthio)-phenyl]pyrrolo-[2,1-a]-isoquinoline ([^18^F]FEMcN) was generated and its biodistribution in the mouse brain was investigated by ex vivo autoradiography.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=%5B18F%5DFEMcN+synthesis&WebEnv=0LHqIrPmGbKKKfGgnibw4HonszsH3kfUSadlCC9TWLl9IhO-oo9unciu0tnRjnhyHE3fJeliIo1Cl7%40D475071265C2C690_0024SID&WebEnvRq=1)]

The synthesis of [^18^F]FEMcN was described by Suehiro et al. (5). McN5652 was demethylated in dry dimethylforamide (DMF) with an excess of sodium thiomethoxide. The reaction mixture was then cooled and an excess of 1-bromo-2-fluoroethane was added, with stirring, at room temperature. The resulting product was extracted into dichloromethane and the solvent was evaporated under vacuum. Purification of FEMcN was performed by semipreparative high performance liquid chromatography (HPLC) followed by a dichloromethane extraction. The identity of FEMcN was confirmed by nuclear magnetic resonance and mass spectroscopy. The yield of this reaction was 41%.

The [^18^F]fluorination of FEMcN was done with a two step procedure. To start, 1-Bromo-2-[^18^F]fluoroethane was synthesized from 2-bromoethyl triflate in acetonitrile at room temperature (5). The [^18^F]FEMcN was prepared by S-[^18^F]fluoroethylation of normethyl McN5652 that was formed by hydrolysis of the butyrate thioester precursor with 1-bromo-2-[^18^F]fluoroethane. Hydrolysis of the thioester was performed as described by Suehiro et al. (9). Tetrabutylammonium hydroxide (1 M in methanol) was added to the thioester precursor in a vial and stirred on a vortex mixer. After 10 min, 0.1 mL DMF was added, and the solution was transferred into the vial containing 1-bromo-2-[^18^F]fluoroethane that had been prepared as described above. The reaction mixture was warmed in a 40-45^o^ C water bath for 1 min, diluted with acetonitrile:water mixture containing 0.1 M ammonium formate and applied to a semi-preparative C-18 column. The radioactive peak with a retention time corresponding to the FEMcN standard was collected. The solvent was evaporated and the residue was dissolved in sterile normal saline. It was then filtered through a 0.22 µM filter into a sterile vial. The radioactive purity and specific activity of the compound were determined by HPLC.

The overall average yield from eleven independent synthesis reactions, based on [^18^F]fluoride, was 13.0 ± 7.1%. The average synthesis time, including HPLC purification and analysis, was 82 ± 12.1 min. The average specific activity of [^18^F]FEMcN was 1593 ± 625 mCi/µmole (58,941 ± 23,125 MBq/ µmole). The time at which the specific activity was measured, radiochemical purity and stability of the product was not provided by the investigators.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=%5B18F%5DFEMcN+in+vitro18F%5BAll+Fields%5D+AND+(FEMcN%5BAll+Fields%5D+AND+(%22in+vitro%22%5BPublication+Type%5D+OR+%22in+vitro%22%5BText+Word%5D))&WebEnv=0VGOUvw35mmgVvKo8fqpQakmj4CQ)]

No publications are currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=%5B18F%5DFEMcN+rodentia&WebEnv=0V4lBsMOGcN0iHZeEU0g6JoaQqctf2qNul3y5f8lIH-QJ_sgsKx1RXmryt6TnaggN9Hka25EuUXoyk%40D475071265C2C690_0024SID&WebEnvRq=1)]

Ex vivo autoradiographic studies on mice revealed that [^18^F]FEMcN accumulated in the high density 5-HT regions of the brain such as hypothalamus, substantia nigra, and raphe nuclei (5). When nitroquipazine, a selective and highly potent 5-HT uptake blocker, was administered to the animals before [^18^F]FEMcN, the accumulation of radioactivity was similar to that observed in regions with low 5-HT uptake (such as the cerebellum), indicating that the radiotracer bound specifically to SERT. The whole brain uptake of [^18^F]FEMcN was 0.94% of the injected dose (%ID)/organ at 30 min. At 60 min post-injection of the label the regional distribution of radioactivity correlated with the distribution of [^11^C]McN5652 reported earlier from the same laboratory (10). At 120 min the uptake was reduced to 0.35% ID/organ. The specific binding of this radiotracer, as determined with and without blocking by a 5-HT specific uptake blocker, showed the distribution of SERT was similar to that observed during in vitro studies indicating SERT could be visualized in vivo with [^18^F]FEMcN. However, compared to the invivo behavior of [^11^C]McN5652, it was concluded [^18^F]FEMcN was a less favorable PET radiotracer for imaging SERT, because of its lower blood-brain barrier penetration and target-to-nontarget ratios.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=%5B18F%5DFEMcN+Non-Primate+Mammals&WebEnv=0UYDBaXWqQh70JVjQI-16Cb7vMKfBFqNxJtUeQaAh3KbCDJQ0ym75rvOhMbPKAoO3KOewYe7XAodZv%40D475071265C2C690_0024SID&WebEnvRq=1)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=%5B18F%5DFEMcN+Non-Human+Primates&WebEnv=0slGaMPddXWOLcgMkDR0f0OKbB32uPTJuOj7aPjpsidbBad3QgOsrjh5Lw2eMj1fCjZKzK0MRYT6Uj%40D475071265C2C690_0024SID&WebEnvRq=1)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=%5B18F%5DFEMcN+Human+Studies&WebEnv=0OioizAfD3GPtujUTZw_H5hkPcdV1qbIqFc2bAQqjuv2IbANknq-mioKGB3yRVII0oVpfP6LKIVtWt%40D475071265C2C690_0024SID&WebEnvRq=1)]

No publications are currently available.

## References

1 Gershon M.D., Tack J. (2007). The serotonin signaling system: from basic understanding to drug development for functional GI disorders. Gastroenterology.
2 Tambour S., Quertemont E. (2007). Preclinical and clinical pharmacology of alcohol dependence. Fundam Clin Pharmacol.
3 Bagdy G., Kecskemeti V., Riba P., Jakus R. (2007). Serotonin and epilepsy. J Neurochem.
4 Halford J.C., Harrold J.A., Boyland E.J., Lawton C.L., Blundell J.E. (2007). Serotonergic drugs : effects on appetite expression and use for the treatment of obesity. Drugs.
5 Suehiro M., Greenberg J.H., Shiue C.Y., Gonzalez C., Dembowski B., Reivich M. (1996). Radiosynthesis and biodistribution of the S-[18F]fluoroethyl analog of McN5652. Nucl Med Biol.
6 Schule C. (2007). Neuroendocrinological mechanisms of actions of antidepressant drugs. J Neuroendocrinol.
7 Suehiro M., Scheffel U., Ravert H.T., Dannals R.F., Wagner H.N. (1993). [11C](+)McN5652 as a radiotracer for imaging serotonin uptake sites with PET. Life Sci.
8 McCann U.D., Szabo Z., Vranesic M., Seckin E., Wand G., Duval A., Dannals R.F., Ricaurte G.A. (2007). Quantitative positron emission tomography studies of the serotonin transporter in humans previously treated with the appetite suppressants fenfluramine or dexfenfluramine. Mol Imaging Biol.
9 Suehiro M., Musachio J.L., Dannals R.F., Mathews W.B., Ravert H.T., Scheffel U., Wagner H.N. (1995). An improved method for the synthesis of radiolabeled McN5652 via thioester precursors. Nucl Med Biol.
10 Suehiro M., Scheffel U., Dannals R.F., Ravert H.T., Ricaurte G.A., Wagner H.N. (1993). A PET radiotracer for studying serotonin uptake sites: carbon-11-McN-5652Z. J Nucl Med.